# [^18^F]Fluoromisonidazole

Chemical name: | 1-(2-Nitro-imidazolyl)-3-[^18^F]fluoro-2-propanol; 1H-1-(3-[^18^F]fluoro-2-hydroxypropyl)-2-nitroimidazole
Abbreviated name: | [^18^F]FMISO
Synonym: | [^18^F]Fluoromisonidazole
Agent Category: | Compound
Target: | Hypoxic cells (macromolecules)
Target Category: | Intracellular reduction and binding
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Other non-primate mammals; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoromisonidazole%5BAll%20Fields%5D)]

Hypoxia in malignant tumors can affect the outcome of anti-cancer treatments. Malignant tumors are relatively resistant to chemotherapy and irradiative therapy because of their lack of oxygen, a potent radiosensitizer. This is the reason for the multitude of efforts to develop methods and imaging techniques for measuring oxygen in tissues. Radiolabeled 2-nitroimidazole compounds have been developed to specifically detect tumor hypoxia, offering a less invasive and less technically demanding alternative to the Eppendorf (oxygen) electrode method. The imaging technique also avoids sampling bias.

[^18^F]Fluoromisonidazole ([^18^F]FMISO) was proposed as a tracer for determining tumor hypoxia in vivo with clinical positron emission tomography (PET) in 1984. Since then, it has become the most widely used nitroimidazole derivate for this technique (1, 2). [^18^F]FMISO has been shown to selectively bind to hypoxic cells both in vitro and in vivo. It is used to quantitatively assess tumor hypoxia in lung, brain, and head-and-neck cancer patients (3, 4) and in the hearts of patients with myocardial ischemia (5, 6).

[^18^F]FMISO is reduced and binds selectively to macromolecules within hypoxic cells. [^18^F]FMISO is relatively hydrophilic and diffuses across cell membranes, showing a passive distribution in normal tissues (4). Because of the slow reaction mechanisms and the absence of active transport of the tracer molecules, the identification and quantification of hypoxic tumor areas necessitate long examination protocols. Also, in severe conditions (pO_2_ ≤ 2-3 mmHg), hypoxia is underestimated by [^18^F]FMISO uptake measurements, possibly because of the existence of a threshold below which the bioreduction and cell uptake of [^18^F]FMISO does not increase any further (7).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoromisonidazole%5BAll%20Fields%5D%20AND%20synthesis%5BAll%20Fields%5D)]

Two main strategies for synthesizing [^18^F]FMISO are reported in the literature: a nucleophilic substitution on a protected precursor (8, 9) or epoxide ring opening; and the production of the intermediate [^18^F]epifluorohydrin, followed by coupling to 2-nitroimidazole (10). Grierson et al. (11) proposed a two-step synthesis producing [^18^F]FMISO with a high yield (40% end of bombardment (EOB)), high purity (>99%), and a specific activity of 37 TBq/mmol. Through this method, the fluoroalkylating agent [^18^F]epifluorohydrin is first obtained by displacing (2R)-(−)glycidyltosylate (GOTS). [^18^F]FMISO is then obtained by reaction of [^18^F]epifluorohydrin with 2-nitroimidazole and further purification through high-performance liquid chromatography (HPLC).

One of the most promising methods seems to be a nucleophilic substitution of the tolysate-leaving group by [^18^F]fluoride on the tetrahydropyranyl-protected precursor 1-(2′-nitro-1′-imidazolyl)-2-O-tetrahydropyranyl-3-O-toluenesulfonylpropanediol (NITTP), with hydrolysis of the protecting group. An automated synthesis of [^18^F]FMISO by this method has been reported in the literature, using either HPLC or Sep-Paks for the purification of the radiotracer (1, 8). The chemical yield obtained when using NITTP was found to be ≤40% (and reproducible), with a radiochemical purity ≥97%, and a specific activity of about 34 TBq/mmol (8).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoromisonidazole%5BAll%20Fields%5D%20AND%20%28%22in%20vitro%22%5BMeSH%20Terms%5D%20OR%20in%20vitro%5BText%20Word%5D%29)]

[^18^F]FMISO uptake was reported in various studies using tumor cell lines such as V-79, EMT-6, RIF-1, and canine osteosarcoma, incubated under hypoxic conditions (7). Those experiments showed in vitro good selectivity of [^18^F]FMISO for hypoxic cells. Reported uptake ratios between hypoxic and normoxic cultures ranged from 12 to 27, depending on the tumor type. In other in vitro studies using V-79, EMT-6(UW), RIF-1, and CaOs-1 cell lines, it was shown that the decreased uptake in hypoxic cells was directly related to increased oxygen concentrations, and that an O_2_ level between 720 and 2300 ppm reduced [^18^F]FMISO binding by 50%, relative to binding under anoxic conditions (12). Studies using Chinese hamster V79-171b spheroids exposed to 50 mM [^3^H]FMISO for 1 to 6 h under aerobic (5% CO_2_ in air), hypoxic (5% CO_2_, 5% O_2_, in N_2_), or anoxic (5% CO_2_ in N_2_) conditions showed that the uptake in anoxic spheroids was similar to that in anoxic cell monolayers. In experiments performed by Casciari et al. (13), [^18^F]FMISO-PET showed a tumor hypoxic fraction of 15%, a value consistent with those obtained from radiation survival assays (17%) and measurements of oxygen consumption (22%).

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoromisonidazole%5BAll%20Fields%5D%20AND%20%22rodentia%22%5BMeSH%20Terms%5D)]

Rodent studies aimed at evaluating tumor hypoxia have been performed using [^18^F]FMISO-PET and by comparing the obtained results with those from immunohistochemical (IHC) staining techniques. In studies on WAG/Rij rats bearing transplanted syngeneic rhabdomyosarcoma (R1) tumors, a statistically significant correlation (P < 0.05) was obtained between the hypoxic volumes defined with [^18^F]FMISO-PET and the volumes derived from the pimonidazole-stained tumor sections (r = 0.9066; P = 0.0001), regardless of the selected threshold between 1.4 and 2.2. A heterogeneous distribution of hypoxia was observed both with histology and [^18^F]FMISO autoradiography (2). Biodistribution studies by Rasey et al. (14) showed that 36% and 57% of [^18^F]FMISO-derived activity was metabolized at 2 and 4 h after injection, respectively.

Rodent studies such as the one by Rasey et al. (15) on 36B10 rat gliomas determined the radiobiologically hypoxic fraction from radiation response data using the paired cell survival curve technique (method 1) in comparison with mathematical modeling of time-activity data (method 2) acquired by [^18^F]FMISO-PET uptake. The radiobiologically hypoxic fraction determined for tumors in air-breathing rats during imaging was 6.1% (95% CL, 4.3-8.6%). A comparable value was obtained by modeling [^18^F]FMISO time-activity data (7. 4%; 95% CL, 2.5-17.3%). In contrast, the two methods led to different values for rats breathing 10% oxygen. In that case, the hypoxic fraction determined by the first method was 13.1% (95% CL, 7.9-8.3%), 43% lower than the value obtained by method 2. The authors suggested that such a discrepancy might be attributable in large part to the inability of [^18^F]FMISO to identify hypoxic cells at pO_2_ ≤ 2-3 mm Hg.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoromisonidazole%5BAll%20Fields%5D%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoromisonidazole%5BAll%20Fields%5D%20AND%20%28dog%20OR%20pig%29)]

Several pig and dog studies aimed at quantifying the relationship between [^18^F]FMISO uptake and the hypoxic fraction in tumors were reported in the literature. Piert et al.(16) found a negative exponential relationship between liver standardized uptake values (SUVs) and the oxygen pressure in the liver of domestic pigs. They determined the activity of [^18^F]FMISO in relation to the hepatic oxygen availability and the partial pressure of oxygen in tissue (tPO_2_) to define a critical oxygen delivery on a regional basis. The experimental procedure involved injecting [^18^F]FMISO into pigs 2 h after onset of regional liver hypoxia caused by the occlusion of the branches of the hepatic artery. The fractional concentration of inspired oxygen (FiO_2_) was set to 0.67 in a first group of animals and to 0.21 in a second group. The SUV for [^18^F]FMISO was calculated from tissue samples obtained 3 h after the injection of [^18^F]FMISO (about 10 MBq/kg body weight) and compared with the regional total hepatic oxygen delivery (DO_2_) calculated from the regional arterial and portal venous flow and the oxygen content of the arterial and portal venous blood. Results showed a significant decrease of DO_2_ in occluded liver tissue samples (first group: 0.063 (0.044-0.089); second group: 0.046 (0.032-0.066)) compared with normal flow segments (first group: 0.177 (0.124-0.252); second group: 0.179 (0.128-0.25) ml x min(-1) x g(-1); geometric mean (95% confidence limits): P < 0.01 in the first group and P < 0.001 in the second group). The tPO_2_ of occluded segments (first group: 5.1 (3.2-8.1); second group: 3.9 (2.4-6.2) mm Hg) showed a substantial decrease compared with normal flow segments (first group: 20.2 (12.6-32.5); second group: 22.4 (14.3-35.2) mm Hg; P < 0.01 in first group and P < 0.001 in second group (17)).

Comparative studies of [^18^F]FMISO and [^18^F]fluorodeoxyglucose (FDG) on dogs with viable myocardium were reported in the literature (18). Ex vivo analysis of both ischemic and normal heart tissue showed that FMISO uptake was consistently greater than FDG uptake, and that when analyzed relative to endocardial-epicardial location, endocardial FMISO uptake was significantly greater in all hypoperfused samples.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoromisonidazole%5BAll%20Fields%5D%20AND%20%22humans%22%5BMeSH%20Terms%5D)]

[^18^F]FMISO has been used in humans to assess hypoxia and perfusion in brain tumors. Data obtained by Bruehlmeier et al. (4) using [^18^F]FMISO-PET and [^15^O]H_2_O on patients with glioblastoma showed a positive correlation between [^18^F]FMISO tumor uptake at 0-5 min after injection and [^15^O]H_2_O, with r values between 0.42 and 0.86. No relation between [^18^F]FMISO uptake and perfusion was found at 150-170 after injection. Despite the nature of the covalent binding of [^18^F]FMISO metabolites (19), a degree of reversibility of [^18^F]FMISO tumor binding was reported by Bruehlmeier et al., who suggested this might be attributable to a limited “back diffusing” effect from the cells.

[^18^F]FMISO-PET human studies, including comparative studies using both [^18^F]FMISO and FDG (20), showed that [^18^F]FMISO uptake varied greatly, depending on the tumor types and the tumor sites in the same patient (21, 22). Generally, increased [^18^F]FMISO tumor uptake was found in tumor margins rather than in the centers (4).

[^18^F]FMISO-PET has also been used as a noninvasive method to assess tumor hypoxia in humans with head-and-neck cancer (HNC) and non-small cell lung cancer (NSCLC). In a reported study (3) involving 40 patients with advanced HNC (n = 26) or NSCLC (n = 14) before curative radiotherapy, dynamic (0-15 min) and static PET scans were performed over a 4-h time period after injection. SUVs and ratios-to-reference tissues (mediastinum or muscle) were calculated. Results for HNC showed that patients with local recurrence could be separated from disease-free patients by SUV, 4 h after injection (SUV > 2 for all recurrences). On the other hand, for NSCLC, no similar correlation was observed. The tumor-to-muscle ratios (T/Mu) and tumor-to-mediastinum ratios (T/Me) at 4 h after injection correlated with the risk of relapse in both tumor entities: all patients with a T/Me > 2.0 (NSCLC, n = 5) or with a T/Mu > 1.6 (HNC, n = 5) had tumor recurrence, whereas only 3 of the remaining 11 patients experienced a recurrence (27%).

A variety of compartment models using human [^18^F]FMISO-PET data have been proposed to quantify tumor hypoxia. In 2005, Thorwarth et al. (23) developed a model based on dynamic HNC patient data. This model takes into account the variations of tumor vasculature obtained by immunohistochemical studies and the slow uptake of severely hypoxic and necrotic tissues overlooked by previous models based on SUVs (24).

## References

1 Tang G., Wang M., Tang X., Gan M., Luo L. (2005). Fully automated one-pot synthesis of [(18)F]fluoromisonidazole. Nucl Med Biol.
2 Dubois L., Landuyt W., Haustermans K., Dupont P., Bormans G., Vermaelen P., Flamen P., Verbeken E., Mortelmans L. (2004). Evaluation of hypoxia in an experimental rat tumour model by [(18)F]fluoromisonidazole PET and immunohistochemistry. Br J Cancer.
3 Eschmann S.M., Paulsen F., Reimold M., Dittmann H., Welz S., Reischl G., Machulla H.J., Bares R. (2005). Prognostic impact of hypoxia imaging with 18F-misonidazole PET in non-small cell lung cancer and head and neck cancer before radiotherapy. J Nucl Med.
4 Bruehlmeier M., Roelcke U., Schubiger P.A., Ametamey S.M. (2004). Assessment of hypoxia and perfusion in human brain tumors using PET with 18F-fluoromisonidazole and 15O-H2O. J Nucl Med.
5 Markus R., Reutens D.C., Kazui S., Read S., Wright P., Pearce D.C., Tochon-Danguy H.J., Sachinidis J.I., Donnan G.A. (2004). Hypoxic tissue in ischaemic stroke: persistence and clinical consequences of spontaneous survival. Brain.
6 Guadagno J.V., Donnan G.A., Markus R., Gillard J.H., Baron J.C. (2004). Imaging the ischaemic penumbra. Curr Opin Neurol.
7 Couturier O., Luxen A., Chatal J.F., Vuillez J.P., Rigo P., Hustinx R. (2004). Fluorinated tracers for imaging cancer with positron emission tomography. Eur J Nucl Med Mol Imaging.
8 Kamarainen E.L., Kyllonen T., Nihtila O., Bjork H., Solin O. (2004). Preparation of fluorine-18-labelled fluoromisonidazole using different synthesis methods. J Label Compd Radiopharm.
9 Patt M., Kuntzsch M., Machulla H.J. (1999). Preparation of [18F]fluoromisonidazole by nucleophilic substitution on THP-protected precursor: yield dependence on reaction parameters. J Radioanal Nucl Chem.
10 Jerabeck, P.A., T.B. Patrick, M.R. Kilbourn, D.D. Dischimo, and M.J. Welch, Synthesis and biodistribution of 18F-labeled fluoronitroimidazoles: potential in vivo markers of hypoxic tissue. Int J Radiat Appl Instrum [A], 1986(37): p. 599–605.
11 Grierson J.R., Link J.M., Mathis C.A., Rasey J.S., Krohn K.A. (1989). A radiosynthesis of fluorine-18 fluoromisonidazole. J Nucl Med.
12 Rasey J.S., Nelson N.J., Chin L., Evans M.L., Grunbaum Z. (1990). Characteristics of the binding of labeled fluoromisonidazole in cells in vitro. Radiat Res.
13 Casciari J.J., Rasey J.S. (1995). Determination of the radiobiologically hypoxic fraction in multicellular spheroids from data on the uptake of [3H]fluoromisonidazole. Radiat Res.
14 Rasey J.S., Hofstrand P.D., Chin L.K., Tewson T.J. (1999). Characterization of [18F]fluoroetanidazole, a new radiopharmaceutical for detecting tumor hypoxia. J Nucl Med.
15 Rasey J.S., Casciari J.J., Hofstrand P.D., Muzi M., Graham M.M., Chin L.K. (2000). Determining hypoxic fraction in a rat glioma by uptake of radiolabeled fluoromisonidazole. Radiat Res.
16 Piert M., Machulla H., Becker G., Stahlschmidt A., Patt M., Aldinger P., Dissmann P.D., Fischer H., Bares R., Becker H.D., Lauchart W. (1999). Introducing fluorine-18 fluoromisonidazole positron emission tomography for the localisation and quantification of pig liver hypoxia. Eur J Nucl Med.
17 Piert M., Machulla H.J., Becker G., Aldinger P., Winter E., Bares R. (2000). Dependency of the [18F]fluoromisonidazole uptake on oxygen delivery and tissue oxygenation in the porcine liver. Nucl Med Biol.
18 Caldwell J.H., Revenaugh J.R., Martin G.V., Johnson P.M., Rasey J.S., Krohn K.A. (1995). Comparison of fluorine-18-fluorodeoxyglucose and tritiated fluoromisonidazole uptake during low-flow ischemia. J Nucl Med.
19 Casciari J.J., Graham M.M., Rasey J.S. (1995). A modeling approach for quantifying tumor hypoxia with [F-18]fluoromisonidazole PET time-activity data. Med Phys.
20 Gagel B., Reinartz P., Dimartino E., Zimny M., Pinkawa M., Maneschi P., Stanzel S., Hamacher K., Coenen H.H., Westhofen M., Bull U., Eble M.J. (2004). pO(2) Polarography versus positron emission tomography ([(18)F] fluoromisonidazole, [(18)F]-2-fluoro-2'-deoxyglucose). An appraisal of radiotherapeutically relevant hypoxia. Strahlenther Onkol.
21 Rasey J.S., Koh W.J., Evans M.L., Peterson L.M., Lewellen T.K., Graham M.M., Krohn K.A. (1996). Quantifying regional hypoxia in human tumors with positron emission tomography of [18F]fluoromisonidazole: a pretherapy study of 37 patients. Int J Radiat Oncol Biol Phys.
22 Rajendran J.G., Wilson D.C., Conrad E.U., Peterson L.M., Bruckner J.D., Rasey J.S., Chin L.K., Hofstrand P.D., Grierson J.R., Eary J.F., Krohn K.A. (2003). [(18)F]FMISO and [(18)F]FDG PET imaging in soft tissue sarcomas: correlation of hypoxia, metabolism and VEGF expression. Eur J Nucl Med Mol Imaging.
23 Janssen H.L., Hoebers F.J., Sprong D., Goethals L., Williams K.J., Stratford I.J., Haustermans K.M., Balm A.J., Begg A.C. (2004). Differentiation-associated staining with anti-pimonidazole antibodies in head and neck tumors. Radiother Oncol.
24 Thorwarth D., Eschmann S.M., Paulsen F., Alber M. (2005). A kinetic model for dynamic [18F]-Fmiso PET data to analyse tumour hypoxia. Phys Med Biol.